# Eu-chelate anti-fibrin antibody-conjugated perfluorocarbon nanoparticles

Chemical name: | Eu-chelate anti-fibrin antibody-conjugated perfluorocarbon nanoparticles
Abbreviated name: | EuPFC
Synonym:
Agent category: | Antibody, small molecule (nanoparticle)
Target: | Fibrin
Target category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI), Ultrasound
Source of signal/contrast: | Europium, perfluorocarbon
Activation: | No
Studies: | - In vitro | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=fibrin + paracest)]

Acute thrombus formation after atherosclerotic plaque rupture has been well recognized as the cause of unstable angina, myocardial infarction, transient ischemic attack, and stroke (1, 2). Platelets and fibrin are the major components of all thrombi involved in the development and progression of atherosclerotic disease (3). Magnetic resonance imaging (MRI) has shown promise in thrombus detection in both animals and humans (4), either with direct thrombus imaging based on the T_1_-shortening properties of endogenous methemoglobin in venous thrombi (5) or by enhancement of the contrast between the myocardium and intracardiac tissues by conventional gadolinium (Gd) chelates (6). However, thrombosis is a dynamic process in which thrombus material of different ages forms a layered structure as a result of successive mural deposition (7). The MRI signal of a thrombus is complicated by the presence of platelets, fibrin, and red blood cells in the clots (7). Accurate thrombus age definition and detection of old and organized thrombi remain difficult. Because fibrin is abundant in all types of thrombi, including arterial, venous, acute, and chronic, contrast agents that target fibrin can be used to differentiate between layers of fibrin deposits in all types of thrombi and in superimposed thrombosis associated with plaque (3). Fibrin is formed after thrombin cleavage of fibrinopeptide A from fibrinogen Aα-chains, followed by polymerization and cross-linkage to form thick fibrin bundles and complex, branched-clot networks (8). The low concentration of fibrin present in plasma minimizes spurious background imaging signals (3).

Europium(III) (Eu^3+^) is a lanthanide cation with six unpaired electrons in the f-shell. Many of the physical and chemical properties of Eu^3+^ are similar to those of its neighbor Gd(III) (Gd^3+^), which has seven unpaired electrons. However, the spin interactions between Eu^3+^ and its directly bound water molecules are quite different from the spin interactions between Gd^3+^ and its directly bound water molecules. Both Gd^3+^ and Eu^3+^ exhibit a large effective magnetic momentum to generate a paramagnetic effect. The electron relaxation time of Eu^3+^ (10^-12^–10^-13^ s) is between four and five orders of magnitude shorter than that of Gd^3+^ (10^-8^–10^-9^s) (9). The pseudocontact shift is quite large for Eu^3+^, but it is zero for Gd^3+^ (9). As a result, Gd chelates are used as T_1_-relaxation agents in MRI because of a strong enhancement effect in T_1_ relaxation; Eu chelates are used as a chemical shift agent in nuclear magnetic resonance spectroscopy because they induce a substantial chemical shift effect. Eu^3+^ has a negligible effect on water proton T_1_ relaxivity because of its short electron relaxation time (9, 10). Similar to Gd-1,4,7,10-tetraazcyclododecane-N,N’,N”,N”’-tetraacetate (Gd-DOTA), Eu-DOTA has one coordinated water molecule in exchange with bulk water. The water residual time (τ_m_) can be prolonged to sub-millisecond scale by substitution of DOTA with various hydrophilic groups that drag the water exchange kinetics into slow exchange region (Δωτ_m_ >>1) (11). Here Δω is the chemical shift difference between water molecules bound to the metal cation and bulk water, and its value is ~50 ppm for Eu^3+^ (12, 13). Radiofrequency prepulses applied at the appropriate frequency and power level can saturate Eu^3+^-bound water molecules. The exchange between the bound water and the bulk water pool leads to reduced equilibrium magnetization for bulk water (11). This negative imaging contrast, called paramagnetic chemical exchange saturation transfer (PARACEST) contrast (11), is “switched on” by simply changing the pulse sequence parameters, a unique feature of MRI. Simultaneously, the prepulse also generates magnetization transfer (MT) effect between the exchangeable protons in tissues (-NH, -OH, etc.) with bulk water. The MT effect produces a magnetization profile (Z-spectrum) of bulk water that is symmetrical about the chemical shift of bulk water (14, 15). Thus, a net change that originated from the PARACEST effect can be obtained by subtraction of images collected at ± frequency offset of the presaturation pulses. In general, signal change in bulk water is 37% for ~100 μM PARACEST agent and 5% for ~10 μM PARACEST agent (11). A major advantage of PARACEST contrast is easy detection of the targeted agent without the need to collect images before and after contrast administration (16).

Eu chelate anti-fibrin antibody–conjugated perfluorocarbon (PFC) nanoparticles (EuPFC) are a MRI PARACEST agent used to image fibrin (16). EuPFC consists of three components (i.e., biotinylated phospholipids, Eu chelate–conjugated phospholipid, and monolayer lipid-encapsulated PFC nanoparticles). The biotinylated phospholipids provide convenience for site-directed targeting. The PFC nanoparticle has a liquid core that is ~200–250 nm in diameter and is emulsified through a microfluidization technique at 20,000 psi. Historically, PFC emulsions have been used as blood substitutes as a result of its high O_2_-loading capacity and excellent biological inertness (17). Recently, PFC emulsions have been adopted for use as principal components in ultrasound contrast agents because of their low acoustic impedance relative to that of soft tissues (18). Unlike microbubble-based formulations, the nanoparticles produce a negligible signal in circulation until they are bound and concentrated at a specific target. The prolonged systematic half-life of EuPFC (β-elimination time was ~1 h) provides adequate time for the nanoparticles to saturate targeted binding sites (19). The large surface of a PFC can be modified to carry a substantial amount of targeting ligands (antibodies, peptides, biotins) and imaging payloads used in MRI, nuclear imaging, and computed tomography (20). For instance, a PFC nanoparticle can support up to 50,000–100,000 Gd chelates, which allows robust detection of target molecules in the pM range by MRI (20). This also creates a bifunctional ultrasonic contrast agent that can be used in combination with other imaging modalities.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(fibrin + paracest )+AND+synthesis%0D%0A)]

Winter et al. briefly described the synthesis of EuPFC (16). Commercially available 1-(2-methyloxy-5-amine-benzyl)-tetra-glycine ethyl-1,4,7,10 tetraazacyclododecane-1,4,7,10-tetraacetate was coupled to a phosphatidylethanolamine through a thiourea linkage to the amine on the phenyl ring. Eu^3+^ was added at equimolar concentrations to form the PARACEST agent, abbreviated as Eu^3+^-methoxyl-benzyl-DOTA. PFC nanoparticles were obtained by emulsion of 15% (v/v) perfluorooctyl bromide (PFOB, C_8_F_17_Br), 1% (w/v) surfactant co-mixture, 2.5% (w/v) glycerin, and water in a microfluidizer for 4 min at 20,000 psi. The co-mixture was a liposome suspension made from a chloroform solution of 64 mol% lecithin, 35 mol% cholesterol, and 1 mol% N-((6-(biotinoyl)amino)hexanoyl)-dipalmitoyl-L-alpha-phosphatidylethanolamine. The obtained PFC nanoparticles were functionalized with a surfactant comprising phosphatidylcholine, biotinylated dipalmitoylphosphatidylethanolamine, and Eu^3+^-methoxyl-benzyl-DOTA at a molar ratio of 59:1:40. The size of the nanoparticles was measured with electrophoretic light-scattering/laser Doppler velocimetry. The diameter was found to be 294 nm with a distribution of 0.215. The Eu^3+^ content was determined by standard comparator instrumental neutron activation analysis. The concentration of Eu^3+^ in the EuPFC emulsion was 2.1 mM.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(fibrin + paracest)+AND+%22in+vitro%22)]

Winter et al. conducted a series of imaging and spectroscopy studies on a 4.7-T imager (16). First, proton spectra of bulk water were collected for both EuPFC and control PFC nanopartciles using a 2-s presaturation pulse at a power level of 28 dB. The magnetization of bulk water was plotted as a function of frequency offset that ranged from 100 ppm to +100 ppm (relative to the bulk water frequency of 0 ppm. Compared to the control nanoparticles, EuPFC exhibited a marked saturation contrast effect at a presaturation frequency of +52 ppm. Second, the enhancement effect of EuPFC was examined in a two-compartment phantom in which EuPFC and control nanoparticles were located in separate chambers. Images were collected with the use of 2.5-s presaturation pulses at a power level of 38 dB with frequency offset of ±52 ppm relative to the bulk water peak. Subtraction of the images collected with saturation at +52 ppm from the images collected at -52 ppm demonstrated an 11.7% image enhancement in the compartment with EuPFC compared to the control nanoparticles. The enhancement effect of EuPFC was then examined in cylindrical plasma clots suspended in sterile saline. The acellular clots were formed in a plastic mold (5 mm in diameter) by combining fresh dog plasma with 5 U of thrombin and CaCl_2_. Subsequently, the clots were incubated with 150 μg biotinylated anti-fibrin antibodies (1H10) overnight followed by 50 μg avidin for 1 h, then 250 μl of EuPFC for 1 h. The images were acquired with parameters identical to those used for the two-compartment phantom. After the subtraction of the images collected with saturation at +52 ppm from the images collected at -52 ppm, the surface of the clot treated with fibrin-targeted EuPFC appeared to have ~10% enhancement in signal intensity and could be clearly distinguished from the rest.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(fibrin + paracest) +AND+rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(fibrin + paracest) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(fibrin + paracest) +AND+human)]

No publication is currently available.

### NIH Support

CO 07121, HL 42950, HL 59865, EB 01704

## References

1 Libby P. (2001). Current concepts of the pathogenesis of the acute coronary syndromes. Circulation.
2 Briley-Saebo K.C., Mulder W.J., Mani V., Hyafil F., Amirbekian V., Aguinaldo J.G., Fisher E.A., Fayad Z.A. (2007). Magnetic resonance imaging of vulnerable atherosclerotic plaques: current imaging strategies and molecular imaging probes. J Magn Reson Imaging.
3 Sirol M., Aguinaldo J.G., Graham P.B., Weisskoff R., Lauffer R., Mizsei G., Chereshnev I., Fallon J.T., Reis E., Fuster V., Toussaint J.F., Fayad Z.A. (2005). Fibrin-targeted contrast agent for improvement of in vivo acute thrombus detection with magnetic resonance imaging. Atherosclerosis.
4 Yuan C., Kerwin W.S., Yarnykh V.L., Cai J., Saam T., Chu B., Takaya N., Ferguson M.S., Underhill H., Xu D., Liu F., Hatsukami T.S. (2006). MRI of atherosclerosis in clinical trials. NMR Biomed.
5 Viereck J., Ruberg F.L., Qiao Y., Perez A.S., Detwiller K., Johnstone M., Hamilton J.A. (2005). MRI of atherothrombosis associated with plaque rupture. Arterioscler Thromb Vasc Biol.
6 Ala-Korpela M., Sipola P., Kaski K. (2006). Characterization and molecular detection of atherothrombosis by magnetic resonance--potential tools for individual risk assessment and diagnostics. Ann Med.
7 Botnar R.M., Perez A.S., Witte S., Wiethoff A.J., Laredo J., Hamilton J., Quist W., Parsons E.C., Vaidya A., Kolodziej A., Barrett J.A., Graham P.B., Weisskoff R.M., Manning W.J., Johnstone M.T. (2004). In vivo molecular imaging of acute and subacute thrombosis using a fibrin-binding magnetic resonance imaging contrast agent. Circulation.
8 Mosesson M.W. (2005). Fibrinogen and fibrin structure and functions. J Thromb Haemost.
9 Peters J.A., Huskens J., Raber D.J. (1996). Lanthanide induced shifts and relaxation rate enhancements. Prog. NMR Spectrosc.
10 Geraldes C.F. (1993). Lanthanide shift reagents. Methods Enzymol.
11 Zhang S., Merritt M., Woessner D.E., Lenkinski R.E., Sherry A.D. (2003). PARACEST agents: modulating MRI contrast via water proton exchange. Acc Chem Res.
12 Zhang S., Wu K., Biewer M.C., Sherry A.D. (2001). 1H and (17)O NMR detection of a lanthanide-bound water molecule at ambient temperatures in pure water as solvent. Inorg Chem.
13 Zhang S., Winter P., Wu K., Sherry A.D. (2001). A novel europium(III)-based MRI contrast agent. J Am Chem Soc.
14 Wolff S.D., Balaban R.S. (1989). Magnetization transfer contrast (MTC) and tissue water proton relaxation in vivo. Magn Reson Med.
15 Ward K.M., Aletras A.H., Balaban R.S. (2000). A new class of contrast agents for MRI based on proton chemical exchange dependent saturation transfer (CEST). J Magn Reson.
16 Winter P.M., Cai K., Chen J., Adair C.R., Kiefer G.E., Athey P.S., Gaffney P.J., Buff C.E., Robertson J.D., Caruthers S.D., Wickline S.A., Lanza G.M. (2006). Targeted PARACEST nanoparticle contrast agent for the detection of fibrin. Magn Reson Med.
17 Spahn D.R. (1999). Blood substitutes. Artificial oxygen carriers: perfluorocarbon emulsions. Crit Care.
18 Lanza G.M., Wallace K.D., Scott M.J., Cacheris W.P., Abendschein D.R., Christy D.H., Sharkey A.M., Miller J.G., Gaffney P.J., Wickline S.A. (1996). A novel site-targeted ultrasonic contrast agent with broad biomedical application. Circulation.
19 Marsh J.N., Hall C.S., Scott M.J., Fuhrhop R.W., Gaffney P.J., Wickline S.A., Lanza G.M. (2002). Improvements in the ultrasonic contrast of targeted perfluorocarbon nanoparticles using an acoustic transmission line model. IEEE Trans Ultrason Ferroelectr Freq Control.
20 Winter P.M., Cai K., Caruthers S.D., Wickline S.A., Lanza G.M. (2007). Emerging nanomedicine opportunities with perfluorocarbon nanoparticles. Expert Rev Med Devices.